# ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Epidermal growth factor

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Epidermal growth factor
Abbreviated name: | ^68^Ga-DOTA-EGF
Synonym:
Agent category: | Polypeptide
Target: | EGF receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20epidermal%20growth%20factor%20and%20human)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab (a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody against the extracellular domain of recombinant HER2) (11) and C225 (an anti-EGFR, chimeric, monoclonal antibody) have been labeled as ^111^In-trastuzumab (http://www.ncbi.nlm.nih.gov/books/NBK23144/) (12-14) and ^99m^Tc-EC-C225 (http://www.ncbi.nlm.nih.gov/books/NBK23305/) (15, 16) for imaging EGFR expression on solid tumors using single-photon emission computed tomography (SPECT). However, antibodies that are approximately 25-fold larger than EGF may not be easily transported to cells within solid tumors. Therefore, ^111^In-EGF (http://www.ncbi.nlm.nih.gov/books/NBK23715/) and ^99m^Tc-HYNIC-EGF (http://www.ncbi.nlm.nih.gov/books/NBK23264/) have been developed for SPECT imaging studies of tumors (17, 18). However, positron emission tomography (PET) offers better sensitivity, resolution, and quantification than SPECT (19). ^68^Ga (t_1/2_ = 68 min, 89% β^+^ decay) is an attractive radionuclide for labeling EGF and is readily available from a commercial ^68^Ge/^68^Ga generator. Cells retain ^68^Ga well, providing a good signal/background ratio. For evaluation as a PET imaging agent, ^68^Ga has been attached to EGF via 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to form ^68^Ga-DOTA-EGF (20).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in OMIM (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20epidermal%20growth%20factor%20and%20synthesis)]

Commercially available monofunctional N-hydroxysuccinimide ester of DOTA was used to conjugate human EGF to form DOTA-EGF, which was purified by column chromatography (20). ^68^Ga was conjugated to DOTA-EGF under microwave heating for 1 min to 95°C. ^68^Ga-DOTA-EGF was purified by column chromatography. The yield of ^68^Ga-DOTA-EGF was 60–77% with a radiochemical purity >95% and specific activities of 12–20 MBq/nmol (0.32–0.54 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20epidermal%20growth%20factor%20and%20in%20vitro)]

Velikyan et al. (20) performed cell-binding assays with ^68^Ga-DOTA-EGF using EGFR-expressing human cervical carcinoma A431 and glioma U343 cell lines. Binding of ^68^Ga-DOTA-EGF (approximately 0.01 μM) to both cell lines was completely blocked by EGF (approximately 1 μM). Saturation binding experiments determined that dissociation constant (K_d_) values were 2.0 and 2.3 nM for A431 and U343 cells, respectively. The number of binding sites per cells was 1.9 × 10^6^ per A431 cell and 7.8 × 10^5^ per U343 cell. Both cell lines rapidly internalized ^68^Ga-DOTA-EGF at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20epidermal%20growth%20factor%20and%20rodentia)]

Velikyan et al. (20) studied the biodistribution of ^68^Ga-DOTA-EGF in nude mice bearing an A431 xenograft. The organs with the highest accumulation at 30 min after ^68^Ga-DOTA-EGF injection were the kidneys and liver (>35%ID/g), followed by the pancreas, salivary gland, small and large intestines, stomach, and spleen. The uptake of ^68^Ga-DOTA-EGF in the A431 tumor xenograft was 1.51 ± 0.16 and 2.69 ± 0.29%ID/g for 0.016 and 0.16 nmol ^68^Ga-DOTA-EGF, respectively (P = 0.036). The radiotracer had a rapid blood clearance at 30 min with tumor/blood ratios of 4.42 ± 1.81 and 4.50 ± 2.53 for 0.016 and 0.16 nmol ^68^Ga-DOTA-EGF, respectively. Very high radioactivity was found in bile, urine, and feces. No blocking experiment was performed.

The whole-body distribution of ^68^Ga-DOTA-EGF (2.0 MBq/mouse or 0.05 mCi/mouse) was also assessed by PET imaging from 20–30 min after injection. The highest activity concentrations were visualized in the kidneys and liver with clearance of radioactivity through the urinary bladder. The accumulation of ^68^Ga-DOTA-EGF was clearly visible in the tumors. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20epidermal%20growth%20factor%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20epidermal%20growth%20factor%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20epidermal%20growth%20factor%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
16 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
17 Cornelissen B., Kersemans V., Burvenich I., Oltenfreiter R., Vanderheyden J.L., Boerman O., Vandewiele C., Slegers G. (2005). Synthesis, biodistribution and effects of farnesyltransferase inhibitor therapy on tumour uptake in mice of 99mTc labelled epidermal growth factor. Nucl Med Commun.
18 Reilly R.M., Kiarash R., Sandhu J., Lee Y.W., Cameron R.G., Hendler A., Vallis K., Gariepy J. (2000). A comparison of EGF and MAb 528 labeled with 111In for imaging human breast cancer. J Nucl Med.
19 Lundqvist H., Tolmachev V. (2002). Targeting peptides and positron emission tomography. Biopolymers.
20 Velikyan I., Sundberg A.L., Lindhe O., Hoglund A.U., Eriksson O., Werner E., Carlsson J., Bergstrom M., Langstrom B., Tolmachev V. (2005). Preparation and evaluation of (68)Ga-DOTA-hEGF for visualization of EGFR expression in malignant tumors. J Nucl Med.